# Gold nanoparticles functionalized with gadolinium-diethylenetriamine pentaacetic acid-cysteine conjugate

Chemical name: | Gold nanoparticles functionalized with gadolinium-diethylenetriamine pentaacetic acid-cysteine conjugate
Abbreviated name: | Au@GdL
Synonym:
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Multimodality imaging (magnetic resonance imaging/computed tomography (MRI/CT))
Source of signal / contrast: | Au and Gd(III)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=multimodality+imaging+and+review)]

The gold nanoparticles (AuNPs) functionalized with the gadolinium (Gd(III))-diethylenetriamine pentaacetic acid (DTPA) conjugate of cysteine, abbreviated as Au@GdL, are a magnetic resonance imaging (MRI)/computed tomography (CT) dual-imaging agent synthesized by Park et al. for MRI/CT multimodality imaging of tumors (1).

Development of hybrid imaging technology has triggered great effort in probe development to boost the benefits of hybrid instrument technology (2-4). In contrast to other agents, multimodal imaging agents for MRI/CT have rarely been explored, although MRI and CT are frequently applied to the same patients for precise diagnosis and treatment evaluation (5-7). Recently, AuNPs have been shown to induce strong contrast enhancement as X-ray contrast agents (8, 9). These particles exhibit a higher X-ray absorption coefficient than iodinated compounds (5.16 and 1.94 cm^2^/g, respectively, at 100 keV). Furthermore, AuNPs are easily controlled with regard to size, shape, and surface modification (1). Gd(III) also possesses a higher X-ray absorption coefficient (3.11 cm^2^/g at 100 keV) than iodine, although this value is lower than that of gold. Interestingly, when Gd(III) ions are bound to NPs, they exhibit a much higher relaxivity than that of clinically approved Gd(III)-chelates (1, 8). Sanchez et al. have shown that the water-soluble apoferritin-encapsulated gadolinium oxide-hydroxide NPs (Gd-Apoferritin) exhibit 10 and 70 times higher T1 and T2 relaxivity values, respectively, than those of classic Gd(III)-complexes (Omniscan^®^ and Gd-DTPA) (8).

On the basis of these facts, Gd(III)-coated AuNPs have been hypothesized to be an efficient dual agent for MRI/CT imaging. Alric et al. demonstrated that Gd(III) chelate-coated AuNPs (Au@DTDTPA-Gd_50_) provide strong X-ray absorption and R1 relaxivity (9). Approximately 50.7 mM Au@DTDTPA-Gd_50_ NPs (10 mg Au/ml) exhibits X-ray absorption equivalent to that of 280 mM iodine (35 mg iodine/ml). The R1 relaxivity of the particles as low as 5 mM Gd(III) is nearly the same as that of Omniscan^®^ (3.90 mM^-1^s^-1^). These particles are small enough (2–2.5 nm) to circulate freely in the blood vessels without undesirable accumulation in organs such as lungs, spleen, and liver. Recently, Park et al. developed a similar MRI/CT dual-imaging agent with Gd(III) and gold reporters (Au@GdL) (1). Au@GdL was generated by encapsulating the gold core within a multilayered organic shell. The contrast enhancement in the MRI stem is from the Gd(III) entrapped in the shell, whereas the gold core provides strong X-ray absorption. Studies by Park et al. showed that Au@GdL had a long circulation time in blood and accumulated within tumor xenografts in animals (1). This chapter summarizes the data obtained with Au@GdL in MRI/CT imaging.

### Related Resource Links:

- Multimodality imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=multimodality%5bAll+Fields%5d+OR+multimodal%5bAll+Fields%5d+AND+micad%5bbook%5d)
- Multimodality imaging clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=multimodality+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20188545)]

Park et al. described the synthesis of Au@GdL in detail (1). The ligand (L), a conjugate of DTPA with cysteine, was prepared by the reaction of DTPA-bis(anhydride) with cysteine at 80°C for 6 h. The subsequent reaction of L with Gd_2_O_3_ for 6 h at 90°C led to the formation of GdL. The coating of AuNPs with GdL was accomplished by direct addition of GdL to citrate-coated AuNPs (~12 nm in diameter) with stirring for 24 h. Au@L NPs without Gd(III) were also synthesized similarly.

The Au@GdL NPs were well dispersed and spherical in shape with a mean diameter of 14 nm and a narrow size distribution. The total number of GdL per AuNP was ~2.9 × 10^3^, which was further confirmed by the weight loss of 5.6% in the temperature range 100–800°C. A higher degree of oligomerization of thiols in L may be a partial explanation for such a high loading of Gd(III). The zeta potential of Au@GdL in water was −41.03 mV at pH 6.0, which was negatively large enough to ensure colloidal stability.

Both Au@GdL and Au@L exhibited greater X-ray attenuation than Ultravist^®^, an iodine-based CT agent used in the clinic, and the differences became greater as the concentration increased. At a concentration of 200 mM, both Au@GdL and Au@L showed attenuation almost three times greater than that of Ultravist^®^. When the comparison was made between Au@GdL and Au@L, the former showed greater attenuation, demonstrating a synergistic effect of Gd(III). An additional contrast enhancement of ~15% seemed to be contributed by 2% of Gd(III) (weight) bound on AuNPs.

At 293 K and 1.5 T, the R1 relaxivity of GdL (7.5 mM−^1^s−^1^) was twice as high as that of Omniscan^®^ (3.30 mM−^1^s−^1^). The same R1 relaxivity increased dramatically to 17.9 mM−^1^s−^1^ with the formation of Au@GdL. When calculated in terms of the AuNP concentration, the molecular R1 relaxivity was 4.6 × 10^5^. The high relaxivity demonstrated by Au@GdL may partially be rationalized in terms of the slower tumbling motion of GdL on AuNPs due to the formation of a rigid oligomeric framework as a result of disulfide bonds.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20188545)]

The cytotoxicity of Au@GdL was evaluated with 14-day-old chick cornea stroma primary cells and NIH-3T3 mouse embryonic fibroblast cells (1). No obvious decrease in cell viability was observed when the cells were exposed for 24 h in the concentration range of 10–1,000 μM Au@GdL. Instead, the relative cell viability increased with the increase of the Au@GdL concentration, indicating that Au@GdL stimulated the cell proliferation in the given concentration range, which is consistent with the reports in the literature (10).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20188545)]

MRI/CT imaging was performed in mice (n = 6) after intravenous injection of Au@GdL.CT imaging at a dose of 1.75 mmol Au/kg showed clear contrast enhancement in all organs (1). The most dramatic enhancement was observed in the liver. The maximum attenuation in the liver reached up to five times that of pre-injection and maintained that level for up to 6 h after injection. The majority of Au@GdL accumulated in the Kupffer cells of the liver as demonstrated with histological and electron microscopic analysis. Some particles accumulated in the kidney and spleen as a result of glomerular filtration function and macrophage activity, respectively.

In line with the observations from CT imaging, MRI at a dose of 0.03 mmol Gd(III)/kg showed a strong signal enhancement, specifically in the liver (1). In addition, prolonged signal enhancement of the abdominal aorta was observed because of the long-circulating blood pool effect of Au@GdL.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Park J.A., Kim H.K., Kim J.H., Jeong S.W., Jung J.C., Lee G.H., Lee J., Chang Y., Kim T.J. (2010). Gold nanoparticles functionalized by gadolinium-DTPA conjugate of cysteine as a multimodal bioimaging agent. Bioorg Med Chem Lett.
2 Boss A., Bisdas S., Kolb A., Hofmann M., Ernemann U., Claussen C.D., Pfannenberg C., Pichler B.J., Reimold M., Stegger L. (2010). Hybrid PET/MRI of intracranial masses: initial experiences and comparison to PET/CT. J Nucl Med.
3 Cherry S.R. (2006). Multimodality in vivo imaging systems: twice the power or double the trouble?. Annu Rev Biomed Eng.
4 Cherry S.R. (2009). Multimodality imaging: beyond PET/CT and SPECT/CT. Semin Nucl Med.
5 Jennings L.E., Long N.J. (2009). 'Two is better than one'--probes for dual-modality molecular imaging. Chem Commun (Camb).
6 Lee S., Chen X. (2009). Dual-modality probes for in vivo molecular imaging. Mol Imaging.
7 Louie A. (2010). Multimodality imaging probes: design and challenges. Chem Rev.
8 Sanchez P., Valero E., Galvez N., Dominguez-Vera J.M., Marinone M., Poletti G., Corti M., Lascialfari A. (2009). MRI relaxation properties of water-soluble apoferritin-encapsulated gadolinium oxide-hydroxide nanoparticles. Dalton Trans.
9 Alric C., Taleb J., Le Duc G., Mandon C., Billotey C., Le Meur-Herland A., Brochard T., Vocanson F., Janier M., Perriat P., Roux S., Tillement O. (2008). Gadolinium chelate coated gold nanoparticles as contrast agents for both X-ray computed tomography and magnetic resonance imaging. J Am Chem Soc.
10 Connor E.E., Mwamuka J., Gole A., Murphy C.J., Wyatt M.D. (2005). Gold nanoparticles are taken up by human cells but do not cause acute cytotoxicity. Small.